# ^99m^Tc-Ethylenedicysteine-deoxyglucose

Chemical name: | ^99m^Tc-Ethylenedicysteine-deoxyglucose
Abbreviated name: | ^99m^Tc-EC-DG, ^99m^Tc-ECDG
Synonym: | ^99m^Tc-Ethylenedicysteine-D-glucosamine
Agent category: | Compound
Target: | Glucose transporters, hexokinases
Target category: | Transporter, enzyme
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EC-DG%20or%20ECDG))]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals (4, 5).

The phosphorylation of glucose, an initial and important step in cellular metabolism, is catalyzed by hexokinases (HKs) (6). There are four HKs in mammalian tissues (HKI–HKIV). HKI, HKII, and HKIII have molecular weights of ~100,000 each; HKI is found mainly in the brain, and HKII is insulin-sensitive and is found in adipose and muscle cells. HKIV, also known as glucokinase, has a molecular weight of 50,000 and is specific to the liver and pancreas. Most brain HK is bound to mitochondria, enabling coordination between glucose consumption and oxidation. Tumor cells are known to be highly glycolytic because of increased expression of glycolytic enzymes and HK activity (7), which have been detected in tumors from patients with lung, gastrointestinal, and breast cancers. The HKs, by converting glucose to glucose-6-phosphate, help maintain the downhill gradient that results in the transport of glucose into cells through the facilitative glucose transporters (GLUT1–13) (8). GLUT4 and HKII are the major transporters and HK isoforms in skeletal, muscle, heart, and adipose tissue, wherein insulin promotes glucose utilization. HKIV is associated with GLUT2 in liver and pancreatic β cells.

2-Deoxy-D-glucose (2-DG) was first developed to inhibit glucose utilization by cancer cells (9). HKs phosphorylate 2-DG to 2-DG-6-phosphate, which inhibits phosphorylation of glucose. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG) was later developed for molecular imaging studies (10). FDG is moved into cells by glucose transporters and is then phosphorylated by HK to FDG-6-phosphate. FDG-6-phosphate cannot be metabolized further in the glycolytic pathway and remains in the cells. Tumor cells do not contain a sufficient amount of glucose-6-phosphatase to reverse the phosphorylation. The elevated rates of glycolysis and glucose transport in many types of tumor cells, and activated cells enhance the uptake of FDG in these cells relative to other normal cells. Positron emission tomography with [^18^F]FDG has been used to assess alterations in glucose metabolism in the brain, cancer, cardiovascular diseases, Alzheimer’s disease and other central nervous system disorders, as well as infectious, autoimmune, and inflammatory diseases (11-16). Glucosamine and FDG have the amino and fluorine group at position 2 of the sugar, and they are taken up in cells by glucose transporters. Yang et al. (17) developed ^99m^Tc-ethylenedicysteine-deoxyglucose (^99m^Tc-EC-DG) by conjugation of two D-glucosamine (2-amino-deoxyglucose) molecules to ethylenedicysteine for single-photon emission computed tomography (SPECT) imaging activity of glucose transporters and hexokinases in tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Glucose%20transporters%20OR%20hexokinases+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Glucose transporter (http://www.ncbi.nlm.nih.gov/gene/6523), hexokinase (http://www.ncbi.nlm.nih.gov/gene/3099)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=Glucose+transporters+OR+hexokinases)
- Clinical trials (FDG (http://www.clinicaltrials.gov/ct2/results?term=FDG))
- Drug information in FDA (FDG (http://google2.fda.gov/search?q=FDG&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EC-DG%20or%20ECDG)+synthesis)]

EC and glucosamine (1:4 molar ratio) were incubated in the presence of sodium hydroxide, sulfo-N-hydroxysuccinimide, and 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide for 24 h at room temperature (17). EC-DG was isolated from the incubation mixture with dialysis. The structure of EC-DG was verified with mass spectroscopy and nuclear magnetic resonance spectroscopy. EC-DG (50 mg) was mixed with 1.1–1.4 MBq (40–50 mCi) ^99m^Tc-pertechnetate and SnCl_2_. ^99m^Tc-EC-DG had a radiochemical purity of 96% and a specific activity of 18.5 GBq/mmol (0.5 Ci/mmol). ^99m^Tc-EC-DG was stable in dog serum for 0.5–24 h of incubation at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EC-DG%20or%20ECDG)+in+vitro)]

In vitro uptake studies of ^99m^Tc-EC-DG and [^18^F]FDG were performed with human lung tumor A549 cells in culture showing 0.5% and 0.6% incubation dose at 4 h of incubation, respectively. D-Glucose was able to block the uptake of ^99m^Tc-EC-DG in a dose-dependent manner. On the other hand, L-glucose showed no inhibition of the uptake. EC-DG was shown to be phosphorylated in a hexokinase assay. ^99m^Tc-EC-DG showed little effect on [^3^H]thymidine incorporation into the A549 cells (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EC-DG%20or%20ECDG)+rodentia)]

Yang et al. (17) performed ex vivo biodistribution studies of ^99m^Tc-EC-DG and [^18^F]FDG in mice (n = 3/group) bearing A549 xenografts at 0.5 h, 2 h, and 4 h after injection. The accumulation of radioactivity of ^99m^Tc-EC-DG in the tumors was 0.79 ± 0.16% of injected dose per gram (% ID/g) at 0.5 h, 0.42 ± 0.12% ID/g at 2 h, and 0.41 ± 0.16% ID/g at 4 h after injection. The liver had the highest accumulation (5.81% ID/g), followed by the kidney (5.69% ID/g) and spleen (4.21% ID/g) at 2 h after injection. Accumulation of radioactivity in the brain (0.04% ID/g) was low. The concentration in the blood was 1.0% ID/g at 2 h after injection. The tumor/blood, tumor/muscle, and tumor/lung ratios were 0.42, 2.75, and 0.59 at 2 h after injection, respectively. The accumulation of radioactivity of [^18^F]FDG in the tumors was 2.23 ± 0.15% ID/g at 0.5 h, 1.70 ± 0.17% ID/g at 2 h, and 1.61 ± 0.18% ID/g at 4 h after injection. ^99m^Tc-EC-DG exhibited higher tumor/muscle and tumor/brain ratios than [^18^F]FDG. On the other hand, [^18^F]FDG exhibited a higher tumor/blood ratio than ^99m^Tc-EC-DG, with no difference in the tumor/lung ratio. Scintigraphy images were obtained in rats bearing breast tumors at 1, 30, and 120 min after intravenous injection of ^99m^Tc-EC-DG. The smallest tumor size that could be visualized was 3 mm. The tumor/muscle ratios were 1.70, 1.58, and 1.82 for the small tumors and 2.36, 2.41, and 2.88 for the medium tumors at the time points, respectively. Pretreatment with FDG decreased the tumor/muscle ratios by 40%, whereas pretreatment with insulin increased the tumor/muscle ratios by 60%. Little tumor accumulation was observed with ^99m^Tc-EC.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EC-DG%20or%20ECDG)+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EC-DG%20or%20ECDG)+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(EC-DG%20or%20ECDG)+human)]

Human dosimetry was estimated on the basis of SPECT scans after injection of 925 MBq (25 mCi) ^99m^Tc-EC-DG in seven patients with non-small-cell lung cancer (NSCLC) (19). The urinary bladder received the highest dose (0.0247 mGy/MBq (91 mrad/mCi)). Other organs that received high doses were the kidney (0.0123 mGy/MBq (45.6 mrad/mCi)) and lung (0.0056 mGy/MBq (20.7 mrad/mCi)). The effective dose equivalent was 0.0059 mSv/MBq (21.8 mrem/mCi). The blood clearance of ^99m^Tc-EC-DG was rapid with <0.0005% ID at 1 h after injection. The primary lung tumor was visualized in six of the seven patients. The other patient was found to have granuloma, which was detected with [^18^F]FDG. The tumor/blood ratios were 4.0 and 20.5 for ^99m^Tc-EC-DG and [^18^F]FDG, respectively.

## NIH Support

CA16672

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Gurfinkel M., Ke S., Wen X., Li C., Sevick-Muraca E.M. (2003). Near-infrared fluorescence optical imaging and tomography. Dis Markers.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Smith T.A. (2000). Mammalian hexokinases and their abnormal expression in cancer. Br J Biomed Sci.
7 Suolinna E.M., Haaparanta M., Paul R., Harkonen P., Solin O., Sipila H. (1986). Metabolism of 2-[18F]fluoro-2-deoxyglucose in tumor-bearing rats: chromatographic and enzymatic studies. Int J Rad Appl Instrum B.
8 Avril N. (2004). GLUT1 expression in tissue and (18)F-FDG uptake. J Nucl Med.
9 Laszlo J., Humphreys S.R., Goldin A. (1960). Effects of glucose analogues (2-deoxy-D-glucose, 2-deoxy-D-galactose) on experimental tumors. J Natl Cancer Inst.
10 Fowler J.S., Ido T. (2002). Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
11 Phelps M.E. (2000). PET: the merging of biology and imaging into molecular imaging. J Nucl Med.
12 Phelps M.E., Mazziotta J.C. (1985). Positron emission tomography: human brain function and biochemistry. Science.
13 Phelps M.E., Mazziotta J.C., Huang S.C. (1982). Study of cerebral function with positron computed tomography. J Cereb Blood Flow Metab.
14 Rohren E.M., Turkington T.G., Coleman R.E. (2004). Clinical applications of PET in oncology. Radiology.
15 Sokoloff L. (1985). Basic principles in imaging of regional cerebral metabolic rates. Res Publ Assoc Res Nerv Ment Dis.
16 Spence A.M., Mankoff D.A., Muzi M. (2003). Positron emission tomography imaging of brain tumors. Neuroimaging Clin N Am.
17 Yang D.J., Kim C.G., Schechter N.R., Azhdarinia A., Yu D.F., Oh C.S., Bryant J.L., Won J.J., Kim E.E., Podoloff D.A. (2003). Imaging with 99mTc ECDG targeted at the multifunctional glucose transport system: feasibility study with rodents. Radiology.
18 Yang D., Yukihiro M., Yu D.F., Ito M., Oh C.S., Kohanim S., Azhdarinia A., Kim C.G., Bryant J., Kim E.E., Podoloff D. (2004). Assessment of therapeutic tumor response using 99mtc-ethylenedicysteine-glucosamine. Cancer Biother Radiopharm.
19 Schechter, N.R., W.D. Erwin, D.J. Yang, E.E. Kim, R.F. Munden, K. Forster, L.C. Taing, J.D. Cox, H.A. Macapinlac, and D.A. Podoloff, Radiation dosimetry and biodistribution of (99m)Tc-ethylene dicysteine-deoxyglucose in patients with non-small-cell lung cancer. Eur J Nucl Med Mol Imaging, 2009